# [^11^C]2-(Dimethylamino)-N-(5,6-dihydro-6-oxophenanthridin-2-yl)acetamide

Chemical name: | [^11^C]2-(Dimethylamino)-N-(5,6-dihydro-6-oxophenanthridin-2-yl)acetamide
Abbreviated name: | [^11^C]PJ34
Synonym:
Agent Category: | Amino acid
Target: | Poly(ADP-ribose)polymerase-1 (PARP-1)
Target Category: | Binding to PARP-1
Method of detection: | PET
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%5BAll%20Fields%5D%20AND%20%28%22PJ%2034%22%5BSubstance%20Name%5D%20OR%20PJ34%5BText%20Word%5D%29)http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?CMD=search&DB=pubmed]

Cellular death can occur through two different chemical pathways: apoptosis and necrosis. Apoptosis is a highly regulated mechanism involving an externalization process of amino-phospholipids, primarily phosphatidylserine (PS), that normally face the cytoplasm (1). Through this process, PS residues are exposed at the outer plasma membrane and face the extracellular fluid (2). Necrosis, on the other hand, is a chaotic, unregulated mode of cell death followed by invasion of inflammatory cells (3).

Imaging of apoptosis through PS exposure using annexin V has been a growing trend over recent years (4, 5). However, because PS inversion occurs in both necrosis and apoptosis, the imaging strategy of quantifying the exposed PS does not differentiate between necrosis from apoptosis. For that reason, other imaging approaches using targeted pathways that are specific to each mechanism are currently under investigation.

The hyperactivation of poly(ADP-ribose) polymerase 1 (PARP-1) followed by depletion of NAD^+^ pools is thought to be the mechanism taking place specifically during necrosis, and probing PARP-1 activity is currently being investigated as a possible route for imaging and evaluating cellular death through necrosis. The phenanthridinone derivative 2-(dimethylamino)-N-(5,6-dihydro-6-oxophenanthridin-2-yl)acetamide (PJ34) is known to inhibit PARP-1 by competing for the NAD^+^ binding site in the activated form of the enzyme (6, 7). Preliminary studies using PJ34 labeled with ^11^C gave favorable data about the possible use of [^11^C]PJ34 in positron emission tomography studies for imaging tissues undergoing cellular death through necrosis (8).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2811C%29PJ34%20AND%20synthesis)http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=fluoroflumazenil%5BAll%20Fields%5D%20AND%20synthesis%5BAll%20Fields%5D]

[^11^C]PJ34 can be synthesized by reaction of the desmethyl precursor N-(5,6-dihydro-6-oxophenanthridin-2-yl)-2(methylamino)acetamide with the labeling agent [^11^C]methyl iodide ([^11^C]MeI), using sodium hydroxide as a base catalyst. Details of such a procedure were reported by Tu et al. (8) in 2005.

Briefly, synthesis of the precursor was accomplished by treatment of phenanthridin-6(5H)-one with 90% nitric acid in acetic acid to produce the corresponding 2-nitro derivative, which was then reduced with iron in aqueous dimethyl formamide to produce the 2-amino analog. This analog was then condensed with N-BOC-protected sarcosine followed by deprotection with ethanolic HCl to finally give the precursor in an overall yield of 74%. ([^11^C]MeI was obtained from [^11^C]carbon dioxide converted to [^11^C]methane and reacted with iodine in the gas phase at 690 °C).

Tu et al. (8) obtained a radiochemical yield >60% for [^11^C]PJ34 (decay-corrected at end of bombardment (EOB)), and a radiochemical purity >99%. The total synthesis time was 50-55 min. The specific activity of the radiotracer produced was ~74,000 MBq/μmol (2,000 mCi/μmol; decay-corrected at EOB; n = 10).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2811C%29PJ34%20AND%20%28in%20vitro%20OR%20cells%29)]

Tu et al. (8) performed immunochemistry studies to obtain further data supporting previous observations (9, 10) of increased uptake of [^11^C]PJ34 in the pancreas of streptozocin (STZ)-treated rats via hyperactivation of PARP-1. The authors used pancreatic tissue slices in conjunction with a rabbit antibody specific for poly(ADP-ribose) residues formed by the enzymatic activity of PARP-1. Observations showed staining inside the nuclei of cells within pancreatic islets for STZ-treated tissues but no poly(ADP-ribose) staining for control rats.

STZ is used as a model of type 1 diabetes. It is taken up by islet beta cells in the pancreas and causes damage to the DNA, which then leads to hyperactivation of PARP-1. Eventually, the cells are depleted of NAD^+^ and cellular death – via necrosis – eventually follows (9).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2811C%29PJ34%20AND%20rodentia%5BMeSH%5D)http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HOMADAM%20AND%20%22rodentia%22]

Biodistribution studies of [^11^C]PJ34 were performed by Tu et al. (8) in Wistar Furth rats (160-180 g) given an intravenous injection of STZ (80 mg/kg of tissue; ~6.6 MBq (180 μCi) per rat). The animals were sacrificed at 5 and 30 min after injection of the radiotracer, organs of interest were removed, and radioactivity was counted.

Results of the studies showed that in STZ-treated animals, the highest uptakes of [^11^C]PJ34 were in the liver (1.138 ± 0.066% injected dose (ID)/g of tissue at 30 min post injection) and pancreas (1.027 ± 0.109% ID/g of tissue at 30 min post injection), compared with control animals (0.767 ± 0.093% ID/g of tissue for the pancreas and 0.885 ± 0.104% ID/g of tissue for the liver at 30 min post injection). These data reflect previous studies showing that hepatocytes and pancreatic islet cells express the GLUT-2 transporter and can be affected by the DNA damage induced by STZ (9, 10).

The following uptake values at 30 min post injection were also reported by Tu et al. (8): in the heart, 0.498 ± 0.055% ID/g of tissue for STZ-treated rats and 0.445 ± 0.044% ID/g of tissue for control animals; in the muscle, 0.233 ± 0.009% ID/g of tissue for STZ-treated rats and 0.0228 ± 0.016% ID/g of tissue for control animals, and in the lung, 0.814 ± 0.043% ID/g of tissue for STZ-treated rats and 0.755 ± 0.136% ID/g of tissue for control animals.

At 5 min post injection, the uptake values obtained for the liver and pancreas were 2.766 ± 0.439 and 1.812 ± 0.234% ID/g of tissue, respectively, for STZ-treated rats and 1.837 ± 0.367 and 1.150 ± 0.118% ID/g of tissue, respectively, for control animals.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2811C%29PJ34%20AND%20%28dog%20OR%20pig%20OR%20sheep%20OR%20rabbit%29)http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HOMADAM%20AND%20%28dog%20OR%20sheep%20OR%20pig%29]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2811C%29PJ34%20AND%20%28primate%20NOT%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2811C%29PJ34%20AND%20human)]

No publication is currently available.

## References

1 Blankenberg FG, Katsikis PD, Tait JF, Davis RE, Naumovski L, Ohtsuki K, Kopiwoda S, Abrams MJ, Darkes M, Robbins RC, Maecker HT, Strauss HW. (1998). In vivo detection and imaging of phosphatidylserine expression during programmed cell death. Proc Natl Acad Sci U S A.
2 Verhoven B, Schlegel RA, Williamson P. (1995). Mechanisms of phosphatidylserine exposure, a phagocyte recognition signal, on apoptotic T lymphocytes. J Exp Med.
3 de Murcia G, Menissier de Murcia J. (1994). Poly(ADP-ribose) polymerase: a molecular nick-sensor. Trends Biochem Sci.
4 Blankenberg FG, Katsikis PD, Tait JF, Davis RE, Naumovski L, Ohtsuki K, Kopiwoda S, Abrams MJ, Strauss HW. (1999). Imaging of apoptosis (programmed cell death) with 99mTc annexin V. J Nucl Med.
5 Blankenberg F, Ohtsuki K, Strauss HW. (1999). Dying a thousand deaths. Radionuclide imaging of apoptosis. Q J Nucl Med.
6 Soriano FG, Virag L, Szabo C. (2001). Diabetic endothelial dysfunction: role of reactive oxygen and nitrogen species production and poly(ADP-ribose) polymerase activation. J Mol Med.
7 Faro R, Toyoda Y, McCully JD, Jagtap P, Szabo E, Virag L, Bianchi C, Levitsky S, Szabo C, Sellke FW. (2002). Myocardial protection by PJ34, a novel potent poly (ADP-ribose) synthetase inhibitor. Ann Thorac Surg.
8 Tu Z, Chu W, Zhang J, Dence CS, Welch MJ, Mach RH. (2005). Synthesis and in vivo evaluation of [11C]PJ34, a potential radiotracer for imaging the role of PARP-1 in necrosis. Nucl Med Biol.
9 Burkart V, Wang ZQ, Radons J, Heller B, Herceg Z, Stingl L, Wagner EF, Kolb H. (1999). Mice lacking the poly(ADP-ribose) polymerase gene are resistant to pancreatic beta-cell destruction and diabetes development induced by streptozocin. Nat Med.
10 Yamamoto H, Uchigata Y, Okamoto H. (1981). Streptozotocin and alloxan induce DNA strand breaks and poly(ADP-ribose) synthetase in pancreatic islets. Nature.